# [^11^C]meta-Hydroxyephedrine

Chemical name: | [^11^C]meta-Hydroxyephedrine
Abbreviated name: | [^11^C]mHED
Synonym: | (1R,2S)-[^11^C]meta-Hydroxyephedrine; [^11^C]HED; [N-methyl ^11^C]meta-Hydroxyephedrine
Agent Category: | Compound
Target: | Norepinephrine transporter (NET), vesicular monoamine transporter (VMAT), neuronal storage vesicle
Target Category: | Transporter binding and storage in the sympathetic nervous system (SNS)
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine)]

[^11^C]-meta-Hydroxyephedrine ([^11^C]mHED) is a radioligand developed for positron emission tomography (PET) imaging of the sympathetic nervous system (SNS). It is a catecholamine analog labeled with ^11^C, a positron emitter with a physical t_½_ of 20.4 min (1).

Many diseases affect the SNS, and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (2, 3). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter, norepinephrine (NE), which stimulates adrenergic receptors of various effector organs (4). There are different types of adrenergic receptors, and NE stimulates α_1_, β_1_ and certain β_2_ receptors. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released from neurons (5). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (6).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. [^123^I]meta-iodobenzylguanidine ([^123^I]MIBG), a single-photon emission tomography (SPECT) agent, has been developed and used for neuronal imaging. Efforts have been made to develop a posiron-emitting tracer because of the inadequate quantitative information and lower spatial resolution obtained by SPECT imaging with MIBG. [^11^C]mHED was developed based on metaraminol, a synthetic false transmitter analog of NE, that accumulates in nerve terminals in the same way as NE (1, 7). Metaraminol is released by nerve stimulation but only has weak postsynaptic effects. Unlike NE, metaraminol is not metabolized by catechol−O−methyl transferase (COMT). The α methyl group on the side chain of metaraminol also renders the compound resistant to oxidative deamination by monoamine oxidase (MAO). [^11^C]mHED is a metaraminol analog and is a good substrate for the NET. It shares the same neuronal uptake mechanism as NE and is also resistant to metabolism by COMT and MAO. Retention of [^11^C]mHED in the NET-expressing tissue appears to be the result of rapid NET-mediated reuptake of the radiotracer.

## Synthesis

Rosenspire et al. (1) synthesized [^11^C]mHED by direct N-methylation of metaraminol for heart neuronal imaging. The precursor compound, metaraminol free base, was prepared from the commercially available metaraminol bitartrate salt. [^11^C]Methyl iodide obtained from the ^14^N(p.α)^11^C reaction was reacted with metaraminol in dimethylformamide/dimethyl sulfoxide (3:1) at 100 ºC for 5 min. The product was purified by high performance liquid chromatography (HPLC) using a C-18 reverse-phase column. [^11^C]mHED was produced with a specific activity of 33.3 ± 18 GBq/µmol (900 ± 487 Ci/mmol) at the end of synthesis (EOS) and a total synthesis time of 45 min. The corrected radiochemical yield was 40-50%, and the radiochemical purity was >98%. The stereoisomer form prepared by this method was the (−) erythro isomer, 1R,2S-(−)MHED.

Nagren K et al. (8) used [^11^C]methyl triflate to prepare [^11^C]mHED. [^11^C]methyl triflate was prepared by reacting [^11^C}methyl iodide with silver triflate impregnated graphitized carbon at 150-200 ºC. Metaraminol in acetonitrile was reacted with [^11^C]methyl triflate at 60 ºC for 1 min, and the product was purified by reversed-phase HPLC. The study reported a decay-corrected radiochemical yield of 65-75%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine%29%20AND%20in%20vitro)]

DeGrado et al. (9) investigated the retention mechanisms of [^11^C]mHED (specific activity >55,500 GBq/mmol or >1500 Ci/mmol) and interactions with NE in isolated rat hearts. They found a strong uptake process (K_1_ = 2.66 ± 0.39 ml/g/min; n = 5) in the heart and a relatively slow clearance rate (k_2_ = 0.011 ± 0.003 min−^1^). NE appeared to increase the clearance rate (k_2_ = 0.016 ± 0.009 min−^1^ at 5 nM and 0.034 ± 0.016 min−^1^ at 10 nM) without affecting initial uptake rates (K_1_ = 2.81 ± 0.25 ml/g/min at 5 nM and 2.53 ± 0.67 ml/g/min at 10 nM). In the presence of 40 nM desipramine (DMI), a potent inhibitor of NET, [^11^C]mHED uptake was blocked. The study indicated that the uptake and retention of [^11^C]mHED by the heart was specific to sympathetic nerve terminals. Caldwell et al. (6) used isolated perfused rat hearts to demonstrated that an axially distributed blood-tissue exchange model could be used for the quantitation of cardiac presynaptic SNS function with [^11^C]mHED.

Buursma et al. (5) studied the potential of using NET as a reporter gene and [^11^C]mHED as a reporter probe for gene therapy in in vitro cell lines of green monkey kidney (COS-7), human glioma (U373), and the human kidney (HEK293). The cells were transiently transduced with an adenoviral vector (AdTrack-hNET). In all 3 cell lines, [^11^C]mHED cellular uptake was positively correlated with AdTrack-hNET viral titer (r^2^ ≥ 0.949; P < 0.05) and enhanced fluorescence of the green fluorescent protein (as a substitute for a therapeutic gene; r^2^ ≥ 0.965; P < 0.005). Human NET (hNET) protein expression was positively correlated (r^2^ = 0.987, P < 0.0001) with [^11^C]mHED uptake in U373 cells. In the presence of DMI, [^11^C]mHED uptake was reduced to the level in control cells (cells infected with control virus).

## Animal Studies

### Rodents

Rosenspire et al. (1) studied the biodistribution of [^11^C]mHED in rats, using doses of 1850-7400 kBq (50-200 µCi) doses. There was preferential uptake of [^11^C]mHED in organs with rich adrenergic innervation (heart, spleen, and adrenals). The radioactivities (as percentage injected dose per g, (% ID)/g; n = 4) in the heart ventricles, spleen, adrenals, liver, kidney, and blood were 3.46 ± 0.47, 1.42 ± 0.56, 1.30 ± 0.12, 2.01 ± 0.34, 3.81 ± 8.70, and 0.13 ± 0.01, respectively, at 5 min. At 30 min, these values were 2.69 ± 0.10, 1.11 ± 0.08, 0.90 ± 0.20, 2.22 ± 0.19, 0.62 ± 0.10, and 0.07 ± 0.01% ID/g, respectively. Radioactivity cleared more rapidly from the lung than from the liver. The heart/liver and heart/lung ratios were 1.2 and 6.6 at 30 min, respectively. The heart/blood ratios at 5 and 30 min were 26 and 35, respectively. When DMI (10 mg/kg) was given to the rats before [^11^C]mHED administration, the radioactivities (as % ID/g) in the heart ventricles, spleen, and adrenal, as compared to those of the untreated rats, were significantly decreased by 92%, 74%, and 62%, respectively,

Law et al. (10) assessed the biodistribution and metabolism of [^11^C]mHED (specific activity = 15-36 GBq/µmol or 0.41-0.97 Ci/µmol at EOS) in rats with doses of 3-30 MBq (0.08-0.8 mCi)/0.8-1.5 nmol/kg. The radioactivity decreased rapidly in the plasma during the first 2 min and then remained relatively constant for the next 60 min. Uptake in the brain was low. Tissue to plasma ratios (tissue cpm х g−^1^/plasma cpm х g−^1^) for myocardium, liver, lung, kidney. and muscle were 36 ± 2, 22 ± 2, 6.0 ± 0.5, 4.1 ± 0.7, and 1.9 ± 0.2, respectively. Co-injection of unlabeled mHED or metaraminol bitartrate decreased myocardium radioactivity, but not in other tissues. No difference was found between the in vivo binding potential for mHED and metaraminol in the myocardium. Analyses of rat plasma and liver samples revealed 6 radioactive metabolites that were more polar than [^11^C]mHED. No metabolites were detected in myocardium samples. In the plasma, 90% of radioactivity at 2.5 min was [^11^C]mHED, which decreased to 15% at 60 min. In the heart, 99.3% of the radioactivity was [^11^C]mHED and the percentage remained unchanged at 60 min.

Buursma et al. (5) used rats bearing U373 s.c. tumor to study the feasibility of using [^11^C]mHED as a reporter gene probe. Tumor-bearing rats received injections of AdTrack-hNET adenovirus 2 days before [^11^C]mHED imaging. Averaged [^11^C]mHED uptake in hNET- transfected tumors (0.13 ± 0.02% ID/g) was significantly higher (P < 0.05) than in the controls (0.11 ± 0.01% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

A metabolic fate study in guinea pigs showed that most of the radioactivity in the heart, liver and blood remained as [^11^C]mHED at 5 min (1). By 30 min, over 50% of liver radioactivity came from metabolites of [^11^C]mHED but >95% radioactivity in the heart remained as [^11^C]mHED. Caldwell et al. (6) showed the feasibility of using [^11^C]mHED imaging to evaluate the presynaptic cardiac sympathetic function in a dog. Hutchins et al. (11) used [^11^C]mHED PET imaging to study sympathetically denervated canine myocardium in dogs and concluded that regional sympathetic denervation altered oxidative metabolism but not perfusion.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine%29%20AND%20human)]

Schwaiger et al (12) evaluated [^11^C]mHED heart imaging in 6 normal volunteers and 5 patients. The specificity activity of [^11^C]mHED was >37,000 GBq (1,000 Ci)/mmol at EOS, and each patient received a dose of 740 MBq (20 mCi). The heart/blood and heart/lung activity ratios in normal volunteers at 30 min after administration were 5.0 and 4.2, respectively. The myocardial activity retention (as the percentage of initial peak activity) decreased from 43 ± 18% at 1 min to 33 ± 16% at 2 min but remained constant (35 ± 13%) up to 60 min. The retention of radioacetivity in the myocardium was markedly reduced in cardiac transplant patients, retention was with 52 ± 17% of the initial peak value at 1 min and decreased to 26 ± 8% at 2 min and 9 ± 3% at 60 min. Ziegler et al. (13) studied the relationship between regional [^11^C]mHED activity and the functional sympathetic innervation of the left ventricle as measured by heart rate variability spectral analysis in 12 cardiac transplant patients. The study showed regional increases in [^11^C]mHED radioactivity and retention (uptake and storage) in patients who demonstrated functional innervation.

A retrospective study by Pietila et al. (14) of 46 patients with chronic heart failure (CHF) indicated that CHF patients had significantly (P<0.0001) lower retention of [^11^C]mHED (0.184 ± 0.061; retention index = myocardium activity/integral of time-activity curve in plasma) than healthy subjects (0.283 ± 0.044). Patients with poor prognosis (death or transplantation) had even lower retention (0.137 ± 0.041; n = 11). Various other studies have shown the potential clinical utility of [^11^C]mHED in evaluating cardiac sympathetic innervation affected by various diseases [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-HED%20OR%20C-11%20HED%20OR%2011C-mHED%20OR%20n%20methyl%2011c%20meta-hydroxyephedrine%29%20AND%20human%20cardiac%20diseases)].

Shulkin et al. (15) used [^11^C]mHED to image pheochromocytoma in 10 patients with known or suspected pheochromocytoma. The radioactivity was rapidly taken up by the tumors, and most tumors were evident within 2-5 min. The tumor activity was unrelated to plasma catecholamine values at the time of administration. There was also prompt radioactivity localization in the liver and kidney. Whereas the liver activity remained constant, the kidney activity rapidly decreased after 4 min. In a study of 12 patients, Trampal et al. (16) found that the sensitivity, specificity, positive predictive value, negative predictive value, and accuracy of [^11^C]mHED imaging in the detection of pheochromocytoma were 92%, 100%, 100%, 87.5%, and 95%, respectively. In another study (17), neuroblastoma was located by PET imaging with [^11^C]mHED (185 MBq (5 mCi) for children) in 7 patients. Tumor activity was evident in imaging within 5 min after administration.

## NIH Support

NIH HL27555, NIMH 41205-7, NCI-5-P32-CA09015, R01 HL41047-01, R01 HL27555-06, HL 52323, NCI R29 CA54216 01.

## References

1 Rosenspire K.C., Haka M.S., Van Dort M.E., Jewett D.M., Gildersleeve D.L., Schwaiger M., Wieland D.M. (1990). Synthesis and preliminary evaluation of carbon-11-meta-hydroxyephedrine: a false transmitter agent for heart neuronal imaging. J Nucl Med.
2. Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
3. Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
4. Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
5 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
6 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
7 Crout J.R., Alpers H.S., Tatum E.L., Shore P.A. (1964). Release of Metaraminol (Aramine) from the Heart by Sympathetic Nerve Stimulation. Science.
8 Nagren K., Muller L., Halldin C., Swahn C.G., Lehikoinen P. (1995). Improved synthesis of some commonly used PET radioligands by the use of [11C]methyl triflate. Nucl Med Biol.
9 DeGrado T.R., Hutchins G.D., Toorongian S.A., Wieland D.M., Schwaiger M. (1993). Myocardial kinetics of carbon-11-meta-hydroxyephedrine: retention mechanisms and effects of norepinephrine. J Nucl Med.
10 Law M.P., Osman S., Davenport R.J., Cunningham V.J., Pike V.W., Camici P.G. (1997). Biodistribution and metabolism of [N-methyl-11C]m-hydroxyephedrine in the rat. Nucl Med Biol.
11 Hutchins G.D., Chen T., Carlson K.A., Fain R.L., Winkle W., Vavrek T., Mock B.H., Zipes D.P. (1999). PET imaging of oxidative metabolism abnormalities in sympathetically denervated canine myocardium. J Nucl Med.
12 Schwaiger M., Kalff V., Rosenspire K., Haka M.S., Molina E., Hutchins G.D., Deeb M., Wolfe E., Wieland D.M. (1990). Noninvasive evaluation of sympathetic nervous system in human heart by positron emission tomography. Circulation.
13 Ziegler S.I., Frey A.W., Uberfuhr P., Dambacher M., Watzlowik P., Nekolla S., Wieland D.M., Reichart B., Schwaiger M. (1996). Assessment of myocardial reinnervation in cardiac transplants by positron emission tomography: functional significance tested by heart rate variability. Clin Sci (Lond).
14 Pietila M., Malminiemi K., Ukkonen H., Saraste M., Nagren K., Lehikoinen P., Voipio-Pulkki L.M. (2001). Reduced myocardial carbon-11 hydroxyephedrine retention is associated with poor prognosis in chronic heart failure. Eur J Nucl Med.
15 Shulkin B.L., Wieland D.M., Schwaiger M., Thompson N.W., Francis I.R., Haka M.S., Rosenspire K.C., Shapiro B., Sisson J.C., Kuhl D.E. (1992). PET scanning with hydroxyephedrine: an approach to the localization of pheochromocytoma. J Nucl Med.
16 Trampal C., Engler H., Juhlin C., Bergstrom M., Langstrom B. (2004). Pheochromocytomas: detection with 11C hydroxyephedrine PET. Radiology.
17 Shulkin B.L., Wieland D.M., Baro M.E., Ungar D.R., Mitchell D.S., Dole M.G., Rawwas J.B., Castle V.P., Sisson J.C., Hutchinson R.J. (1996). PET hydroxyephedrine imaging of neuroblastoma. J Nucl Med.